# ^99m^Tc-Mercaptoacetyl-Glu-Glu-aptamer specific for tenascin-C

Chemical name: | ^99m^Tc-Mercaptoacetyl-Glu-Glu-aptamer specific for tenascin-C
Abbreviated name: | ^99m^Tc-TTA1
Synonym:
Agent category: | Nucleic acid
Target: | Tenascin-C
Target category: | Nucleic acid binding protein
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal/contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+ TTA1)]

Tenascin-C is a large, adhesive, extracellular matrix (ECM) glycoprotein (>10^3^ kDa) (1) with numerous alterative names such as myotendinous antigen, glioma mesenchymal ECM protein (GMEM), cytotactin, J1-200/220, hexabrachion, and neuronectin (2). Tenascin-C contains six disulphide-linked subunits spread as six arms from a central core (3). Each subunit possesses multiple-function domains, including a cysteine-rich N-terminal domain associated with self-oligomerization, followed by epidermal growth factor (EGF)-like repeats, fibronectin (FN) type III-like repeats, and a fibrinogen-like globular domain at the C-terminus. Consequently, tenascin-C can bind to different cell-surface receptors such as integrins and ECM components (FN). Tenascin-C is found to express specifically in damaged tissues, vascular diseases, and a majority of malignant solid tumors (4).

Aptamers (from the Latin aptus, to fit, and the Greek meros, part or region) are single-stranded or double-stranded oligonucleotides (DNA or RNA) that are modified to bind a variety of targets with high binding affinity and specificity (5). Aptamers typically consist of 20–50 nucleotides (8–15 kDa) with dissociation constants in the range of 10 pM to 10 nM (6). Unlike linear oligonucleotides, which contain genetic information or antisense oligonucleotides that interrupt the transcription of genetic information, aptamers are globular molecules with a shape similar to tRNA and bind to target proteins specifically (7). The modification of the oligonucleotides is carried out through the systematic evolution of ligands by exponential enrichment (SELEX) method, in which specific aptamers are generated against desired small proteins, cells, and tissues (8). In general, aptamers are capable of distinguishing between closely related members of a protein family and between different functional or conformational states of the same protein (6). Aptamers have been used in various clinical trials as alternate therapeutics in cancers (6). For in vivo applications, aptamers can be modified chemically against degradation caused by exonucleases and endonucleases (9).

TTA1 is a 39mer oligonucleotide (13.4 kDa) that binds specifically to human tenascin-C with high affinity (dissociation constant, 5 × 10^-9^ M) (9). To enhance its resistance to blood and tissue nucleases, the structure of TTA1 is modified in several locations (9). All pyrimidine ribonucleotides are replaced with 2’-deoxy-2’-fluoronucleolytic nucleotides, 14 of the 19 purine ribonucleotides are replaced with 2’-deoxy-2’-OMe nucleotides, the 3’ end is blocked with a 3’-3’-thymidine cap for exonuclease protection, a (CH_2_CH_2_O)_6_ spacer is connected between oligonucleotide chains, and a 5’ hexyl-aminolinker is added for bioconjugation of imaging probes. Connecting this aminolinker with radionuclide chelators, technetium-labeled mercaptoacetyl-Glu-Glu (^99m^Tc-MAG_2_), yields the molecular imaging agent ^99m^Tc-mercaptoacetyl-Glu-Glu-aptamer specific for tenascin-C (^99m^Tc-TTA1) (8). ^99m^Tc is a common radioactive label used in single-photon emission computed tomography (SPECT) imaging, and it has a 0.90 gamma branch factor, a 6-h half-life at 140 keV, and a low isotope cost ($0.21/mCi) (10). ^99m^Tc-TTA1 appears to be a promising candidate for imaging of tumors expressing tenascin-C (5).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc+ AAT1)+AND+synthesis%0D%0A)]

The synthesis of ^99m^Tc-TTA1 was conducted in three steps (8). First, TTA1 was prepared according to standard protocols on an oligonucleotide synthesizer with the use of 2’-fluoropyrimidine phosphoramidite monomers, 2’-OMe purine, and (CH_2_CH_2_O)_6_ monomers as building blocks (9). Then, TTA1 was reacted with mercaptoacetyl diglycine (MAG_2_) succinimidyl ester at a molar ratio of 1:5 at pH 9.3, followed by purification with reverse-phase liquid chromatography (8). Finally, the produced TTA1-MAG_2_ was reacted with pertechnetate (185 MBq ^99m^Tc in the presence of SnCl_2_ at pH 8.5 to produce a radionuclide-labeled aptamer, ^99m^Tc-TTA1 (8). The product was purified with spin-dialysis through a 10-kDa cutoff membrane filter. This labeling protocol incorporated 30%-50% of the added ^99m^Tc, with a specific activity of 74-111 MBq/nmol of oligonucleotide. The labeling did not appear to alter the affinity of TTA1 binding to tenascin-C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc + AAT1)+AND+%22in+vitro%22)]

The uptake and localization of TTA1 was examined in tumors with TTA1 labeled with fluorescence dye (TTA1-Red) (5). Nude mice bearing human glioblastoma (U251) tumors (200–350 mg) were injected with TTA1-Red at a dose of 5 nmol (3.25 mg/kg). Mice were euthanized at several time points to extract the tumors for fluorescence microscopic imaging and immunohistochemical analysis. The antibody staining demonstrated an abundant presence of tenascin-C in the tumor stroma, including perivascular distribution. Ten minutes after injection of TTA1-Red, an intense fluorescence was found in the perivascular space; 3 h later, the fluorescence signal was diffused throughout the tumor stoma in a distribution pattern similar to that of tenascin-C in the ECM. Approximately 60% of aptamer in the tumor was found intact, suggesting that the fluorescence signal derived from the labeled aptamers.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc + AAT1) +AND++rodentia)]

The biodistribution of ^99m^Tc-TTA1 was measured with a gamma counter in tumor-bearing mice (5). Nude mice with U251 tumors (200–350 mg) implanted on the flank were used in the study. A mixture of 0.5 nmol ^99m^Tc-TTA1 (37–55.5 MBq) with 4.5 nmol TTA1 was injected into the tail vein. The blood and tissues were collected at several time points for analysis of gamma radioactivity. ^99m^Tc-TTA1 was found to clear from the blood rapidly: it decreased to 18% injected dose/gram of tissue (% ID/g) at 2 min after injection and decreased to 0.1% ID/g at 60 min. Tumor uptake was 5.9 ± 0.6% ID/g at 2 min, 2.7% ID/g at 60 min, and 1.2% ID/g at 17 h. The tumor/blood ratio was ~50 at 3 h and ~180 at 6 h. At 10 min after injection, ^99m^Tc-TTA1 accumulation was found to be 19% ID/g in the kidney, 15% ID/g in the small intestine, and 10% ID/g in the liver. Three hours later, the level of ^99m^Tc-TTA1 was 0.2% ID/g in the kidney, 1–1.55% ID/g in the small intestine, and 35–40% ID/g in the large intestine. These results suggested that ^99m^Tc-TTA1 was cleared from body through the renal pathway (~50%) and the hepatobiliary pathway (~50%). No detectable radioactivity was found in blood, lung, or muscle at 3 h. More than 95% of ^99m^Tc was cleared from body in 24 h. The uptake of ^99m^Tc-TTA1 was examined in a variety of solid tumors (5) such as human tumor xenografts including colon cancer (SW620), breast cancer (MDA-MB-468, MDA-MB-435), rhabdomyosarcoma (A673), and squamous cell carcinoma. The radioactivity was found to be 0.1–1.9% ID/g at 3 h, depending on the tumors. The uptake of ^99m^Tc-TTA1 was further examined in vivo with a gamma camera. Scintigraphic images were collected from mice bearing U251 tumors at the same time point at which images were collected for the biodistribution measurement. The results were consistent with the biodistribution data. No blocking study was reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc + TTA1) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(99mTc + TTA1) +AND+human)]

No publication is currently available.

## References

1 Trebaul A., Chan E.K., Midwood K.S. (2007). Regulation of fibroblast migration by tenascin-C. Biochem Soc Trans.
2 Mackie E.J. (1997). Molecules in focus: tenascin-C. Int J Biochem Cell Biol.
3 Bartsch U. (1996). The extracellular matrix molecule tenascin-C: expression in vivo and functional characterization in vitro. Prog Neurobiol.
4 Orend G., Chiquet-Ehrismann R. (2006). Tenascin-C induced signaling in cancer. Cancer Lett.
5 Ng E.W., Shima D.T., Calias P., Cunningham E.T., Guyer D.R., Adamis A.P. (2006). Pegaptanib, a targeted anti-VEGF aptamer for ocular vascular disease. Nat Rev Drug Discov.
6 Guo K.T., Schafer R., Paul A., Ziemer G., Wendel H.P. (2007). Aptamer-based strategies for stem cell research. Mini Rev Med Chem.
7 Hicke B.J., Stephens A.W. (2000). Escort aptamers: a delivery service for diagnosis and therapy. J Clin Invest.
8 Hicke B.J., Stephens A.W., Gould T., Chang Y.F., Lynott C.K., Heil J., Borkowski S., Hilger C.S., Cook G., Warren S., Schmidt P.G. (2006). Tumor targeting by an aptamer. J Nucl Med.
9 Schmidt K.S., Borkowski S., Kurreck J., Stephens A.W., Bald R., Hecht M., Friebe M., Dinkelborg L., Erdmann V.A. (2004). Application of locked nucleic acids to improve aptamer in vivo stability and targeting function. Nucleic Acids Res.
10 Yang D.J., Kim E.E., Inoue T. (2006). Targeted molecular imaging in oncology. Ann Nucl Med.